# Methyl-[^11^C]-4'-thiothymidine

Chemical name: | Methyl-[^11^C]-4’-thiothymidine
Abbreviated name: | [^11^C]-4DST
Synonym: | 4’-[methyl-^11^C]thiothymidine ([methyl-^11^C]S-dThd)
Agent Category: | Compound
Target: | DNA
Target Category: | Nucleic acids
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure of [^11^C]-DST for more information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=4%27-thiothymidine%5D&cmd=DetailsSearch)]

Most anti-cancer drugs are aimed at curbing the processes of rapid cell proliferation and an increased rate of DNA synthesis, which are both necessary for the progression of all cancers and the development of neoplastic tumors. Usually invasive procedures such as biopsies are used to confirm the presence of malignant tumors, but it can be difficult to take multiple biopsies from a patient if the cancer has metastasized to several different areas of the body (1). Therefore, non-invasive imaging methods that use radiolabeled thymidine analogs (a nucleoside present only in the DNA) in conjunction with positron emission tomography (PET) have been developed to detect tumors and to evaluate the efficacy of anti-cancer treatments in animals and humans (1). Initially, ^11^C-labeled thymidine was developed to visualize cancerous tumors, but this radiolabeled compound is quickly metabolized in the cell and has been determined to have limited application in the clinic (2). Subsequently, ^18^F-labeled PET agents with a thymidine base, such as 3’-deoxy-3’-[^18^F]fluorothymidine ([^18^F]-FLT) and 1-(2’-deoxy-2’-[^18^F]fluoro-β-D-arabinofuranosyl) thymine ([^18^F]-FMAU), were generated and evaluated for the visualization of neoplastic tumors. Among these, FLT is phosphorylated by thymidine kinase 1 (a cytosolic isozyme of thymidine kinase), but the phosphorylated molecule is not incorporated into the cellular DNA and is trapped within the cell (2). Hence, [^18^F]-FLT is considered to be a surrogate marker for the visualization of cell proliferation under in vivo conditions. In addition, this cell proliferation tracer has several limitations that have been discussed elsewhere (3). The second tracer, [^18^F]-FMAU, has to be phosphorylated by thymidine kinase 2 (TK2), a mitochondrial enzyme, before it is incorporated into the DNA (2). However, [^18^F]-FMAU is considered suitable only for the detection of neoplasia in the pelvic region or for visualization of tumors that have metastasized to the bone, because with this radiolabeled compound there is a high retention of label in the liver, kidneys, and the myocardium (2). It has also been reported that there is no correlation between the uptake of a TK2-selective arabinothymidine substrate and the proliferation of cells in a malignant tumor (3).

With the information described above, in an effort to produce an alternative tracer that can be used to visualize tumor proliferation, Toyohara et al. synthesized 4’-thiothymidine (in this molecule, the 4’-oxo of thymidine is substituted with a 4’-sulfur) and showed that its methylated and ^14^C-labeled derivative, 4’-methyl-[^14^C]-thiothymidine ([^14^C]-4DST), accumulated mainly in rapidly proliferating tissues in mice (spleen, duodenum, and thymus), including the xenograft tumors (4). It has also been shown that the label from [^14^C]-4DST is present mainly in the DNA fraction of these tissues. On the basis of these observations, ^11^C-labeled 4’-methyl-thiothymidine ([^11^C]-4DST) was synthesized and evaluated for the visualization of cell proliferation with PET in mice bearing xenograft tumors generated from several different cell lines (3). The biodistribution and use of [^11^C]-4DST for the imaging of brain tumors in humans with PET was investigated in a recent pilot study (5).

### Other Sources of Information

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=FMAU+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials with [^18^F]-FLT (http://clinicaltrials.gov/ct2/results?term=18F-FLT)

Clinical trials with [^18^F]-FMAU (http://clinicaltrials.gov/ct2/results?term=18F-FMAU)

Cell proliferation assay (http://www.invitrogen.com/site/us/en/home/References/protocols/cell-and-tissue-analysis/cell-profilteration-assay-protocols.html) protocols

[^3^H]-Thymidine (http://www.scientistsolutions.com/t3176-%5B3h%5D_thymidine+incorporation+assay+for+rat_1a+cells.html) cell proliferation assay (http://www.scientistsolutions.com/taggingclick.aspx?taggingid=73c4797c-0f70-4bd8-9a10-0e914d456911&historyid=3c4fd675-d22d-44c1-b990-3403c7adf6a7&desturl=http%3a%2f%2fen.wikipedia.org%2fwiki%2fAssay)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5D-4DST%20synthesis&cmd=DetailsSearch)]

The synthesis of [^11^C]-4DST using two different precursors (a 5-trimethylstannyl-precursor (5-TMS) and a 5-tributylstannyl-precursor (5-TBS)) has been described by Toyohara et al. (3). The total time of synthesis with both precursors was 30 min from the end of bombardment, and the radiochemical yields (RCY) with 5-TMS and 5-TBS were reported to be 18.9 ± 4.1% (n = 10 synthetic reactions) and 14.5 ± 2.4% (n = 4 synthetic reactions), respectively. The radiochemical purity (RCP) of [^11^C]-4DST obtained with both precursors was >99% as determined with analytical high-performance liquid chromatography (HPLC). The specific activities of the final product synthesized with 5-TMS and 5-TBS were 47 ± 23 GBq/μmol (1.27 ± 0.62 Ci/μmol; n = 6 determinations) and 121 ± 28 GBq/μmol (3.27 ± 0.75 Ci/μmol; n = 4 determinations), respectively.

In another study, [^11^C]-4DST synthesized with the 5-TBS precursor had a RCP of >99% and a specific activity of >80 GBq/mmol (>2.16 Ci/mmol) (6).

When a palladium-mediated rapid C-[^11^C]methylation reaction was used to synthesized [^11^C]-4DST for animal and human use, the RCY, RCP, and specific activity of the labeled compound were reported to be 93%, ≥99.5%, and 89–200 GBq/μmol (2.4–5.4 Ci/μmol), respectively (7).

For use in humans a modified method was used for the synthesis of [^11^C]-4DST as described by Toyohara et al. (5). Briefly, a solution of tri(o-tolyl)phosphine in N,N-dimethylformamide (DMF) and the precursor in DMF was prepared and mixed with copper chloride, potassium carbonate, and Tris(dibenzylideneacetone)dipalladium. Freshly prepared [^11^C]-methyl iodide was then trapped in the reaction mixture of DMF and the reaction mixture was heated at 80°C for 5 min. [^11^C]-4DST was purified from the reaction mixture with high performance liquid chromatography and collected in a flask containing ascorbic acid, evaporated to dryness, dissolved in 0.9% sodium chloride and sterile filtered for use. The total time of synthesis was 25 min from the end of bombardment and the radiochemical yield and purity of the tracer was 73.4 ± 12.3% (n = 7 reactions) and always >99%, respectively. The specific activity of [^11^C]-4DST was reported to be 313 ± 200 TBq/mmol (8459 ± 5405 Ci/mmol) (n = 9 synthesis reactions)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Methyl-%5B11C%5D-4%25u2019-thiothymidine%20in%20vitro&cmd=DetailsSearch)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Methyl-%5B11C%5D-4%u2019-thiothymidine%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]-4DST was investigated in groups of mice (n = 4–5 animals/group) bearing xenograft tumors derived from EMT-6 (a murine mammary carcinoma cell line), LL (a murine lung cancer cell line), Colon-26 (a murine rectum carcinoma cell line), S-180 (a murine sarcoma cell line), and C6 (rat glioma cell line) cells, respectively (3). The animals were administered a bolus of 37 MBq (1 mCi) [^11^C]-4DST (~0.8 nmol) through the tail vein and euthanized 60 min later. All major organs, including the tumors, were then removed from the animals to determine the amount of radioactivity accumulated in the tissues, and the results were presented as standardized uptake values (SUV). Maximum uptake was observed in the spleen of animals of the various groups (SUVs between 2 and >10), followed by tumors derived from the different cell lines (SUVs between ~2 and ~7) and the thymus (SUVs between 1 and ~3). Non-proliferative tissues from organs such as liver, lung, kidneys, etc., had SUVs of <2. From this study, the investigators concluded that the uptake of [^11^C]-4DST by the tumors was high and selective (3). No blocking studies were reported.

In the same study, the DNA-incorporated SUV (DNA_SUV_) of [^11^C]-4DST was compared to that of 2-[^14^C]-4DST in five different tumor tissues (3). The mean DNA_SUV_ with [^11^C]-4DST was reported to be the same as that of 2-[^14^C]-4DST in the various tumor tissues (Pearson’s correlation coefficient r = 0.96, P < 0.01), indicating that the two tracers had a similar behavior under in vivo conditions.

MicroPET imaging of mice between 60 and 70 min after an injection of [^11^C]-4DST showed that there was high uptake of the tracer in the tumor, bone marrow, intestine, and the urinary bladder (3).

Tsuji et al. evaluated the use of [^18^F]-fluorodeoxy glucose ([^18^F]-FDG), [^18^F]-FLT, and [^11^C]-4DST for the imaging of H226 or 211H mesothelioma (http://www.mesothelioma.cc/?kw=mesothelin&c=google&ad=8162159965&SiteTarget=) cell line tumors (the two cell lines are derived from epithelial mesothelioma (http://www.mesothelioma-aid.org/epithelial.htm) and sarcomatoid mesothelioma (http://www.asbestos.com/mesothelioma/malignant-sarcomatoid.php), respectively) implanted subcutaneously and in the pleural cavity of nude mice (6). Histochemical staining confirmed that, compared to the 211H xenograft tumors, the H226 xenografts produced a very high level of mesothelin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=retrieve&dopt=default&rn=1&list_uids=10232), a protein that is overexpressed in epithelial mesothelioma, ovarian cancer, and some squamous cell carcinomas. The animals (n = 3–6 mice/group) were injected with the respective tracers through the tail vein and euthanized 50 min later. The tumors and all major organs were removed to determine the amount of accumulated radioactivity. Compared to either [^18^F]-FDG or [^18^F]-FLT, a significantly higher uptake of [^11^C]-4DST was observed in the H226 xenografts (P < 0.05). In contrast, the 211H tumors showed a significantly higher (P < 0.01) uptake of [^18^F]-FDG compared to that of [^11^C]-4DST. A similar trend was observed with the tumor/heart and tumor/lung ratios with both of these labeled compounds. The differential uptake of the tracers in the two subtypes of mesothelioma was subsequently confirmed with PET imaging of mice bearing the H226 or 211H cell xenograft tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Methyl-%5B11C%5D-4%u2019-thiothymidine%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Methyl-%5B11C%5D-4%u2019-thiothymidine%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Methyl-%5B11C%5D-4%u2019-thiothymidine%20Human%20Studies&cmd=DetailsSearch)]

Toyohara et al. conducted a pilot study with PET to investigate the biodistribution and brain tumor imaging in humans with [^11^C]-4DST (5). For the biodistribution study, three healthy volunteers were administered an intravenous bolus of 688 ± 47.9 MBq (2.2 ± 0.09 mmol) [^11^C]-4DST, and the individuals were subject to whole-body dynamic PET scans for the next ~125 min as detailed elsewhere (5). From the images it was evident that maximum label was initially present (1–11 min of the scan) in the kidneys, followed by the liver; both organs showed a gradual decline in accumulated label during the subsequent scans (24–34 min and 78–98 min). The bone marrow showed a gradual increase in accumulated radioactivity during the entire period of the scan. Only a moderate amount of the tracer was detected in other proliferative tissues, such as the spleen and the intestines; very little uptake was evident in the non-proliferative tissues, such as the muscles and lungs. These observations indicated that the uptake of [^11^C]-4DST was selective for tissue that had a high proliferation rate (5). The highest absorbed dose was estimated to be in the urinary bladder wall (17.6 ± 2.7 μGy/MBq), followed by the kidneys (17.6 ± 2.7 μGy/MBq), liver (12.4 ± 2.3 μGy/MBq), and spleen (6.9 ± 1.4 μGy/MBq); for all other organs, the dose ranged between 1.9 ± 0.1 μGy/MBq (skin) and 4.7 ± 0.2 μGy/MBq (osteogenic cells). The mean effective dose for the radiochemical was estimated to be 4.2 ± 0.3 μSv/MBq.

To investigate the use of [^11^C]-4DST to visualize tumors in the brain with PET, the presence of tumor masses in six patients was initially confirmed with Gd-magnetic resonance imaging (Gd-MRI) or ^11^C-methionine ([^11^C]-Met) PET as described by Toyohara et al. (5). Each patient was then injected with 528–817 MBq/1.7–10.0 mmol (14.3–22.1 mCi/1.7–10.0 mmol) [^11^C]-4DST, dynamic PET scans were acquired for the next 90 min, and the images from the scans were analyzed as detailed elsewhere (5). There was little uptake of [^11^C]-4DST in the normal brain (the radiolabel is impermeable to the blood–brain barrier), but rapidly growing tumors (earlier visualized with Gd-MRI and [^11^C]-Met PET) were clearly visible (because the blood–brain barrier is disrupted in these patients). Although [^11^C]-Met PET detected all the contrast-enhanced regions visualized with Gd-MRI, a clinically stable tumor visualized with Gd-MRI was not confirmed with [^11^C]-4DST. In addition, the distribution pattern of [^11^C]-Met in the tumor regions was not similar to that of [^11^C]-4DST, even in those tumors that had a high accumulation of this label (5).

HPLC analysis of the plasma and the urine of the individuals revealed that several hydrophilic metabolites of [^11^C]-4DST were produced in the patients, indicating that the radiolabeled compound was metabolized in the human system, although it was shown to be stable in mice (5).

From these studies, the investigators concluded that [^11^C]-4DST was suitable for the imaging of brain tumors with PET; however, because it was evaluated in only a small group of humans, further studies are necessary to confirm the suitability of this labeled compound for application in the clinic (5).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Bading J.R., Shields A.F. (2008). Imaging of cell proliferation: status and prospects. J Nucl Med.
2 Chen K., Chen X. (2011). Positron emission tomography imaging of cancer biology: current status and future prospects. Semin Oncol.
3 Toyohara J., Okada M., Toramatsu C., Suzuki K., Irie T. (2008). Feasibility studies of 4'-[methyl-(11)C]thiothymidine as a tumor proliferation imaging agent in mice. Nucl Med Biol.
4 Toyohara J., Kumata K., Fukushi K., Irie T., Suzuki K. (2006). Evaluation of 4'-[methyl-14C]thiothymidine for in vivo DNA synthesis imaging. J Nucl Med.
5 Toyohara J., Nariai T., Sakata M., Oda K., Ishii K., Kawabe T., Irie T., Saga T., Kubota K., Ishiwata K. (2011). Whole-Body Distribution and Brain Tumor Imaging with 11C-4DST: A Pilot Study. J Nucl Med.
6 Tsuji A.B., Sogawa C., Sugyo A., Sudo H., Toyohara J., Koizumi M., Abe M., Hino O., Harada Y.N., Furukawa T., Suzuki K., Saga T. (2009). Comparison of conventional and novel PET tracers for imaging mesothelioma in nude mice with subcutaneous and intrapleural xenografts. Nucl Med Biol.
7 Koyama H., Siqin Z. (2011). Zhang, K. Sumi, Y. Hatta, H. Nagata, H. Doi, and M. Suzuki, Highly efficient syntheses of [methyl-11C]thymidine and its analogue 4'-[methyl-11C]thiothymidine as nucleoside PET probes for cancer cell proliferation by Pd(0)-mediated rapid C-[11C]methylation. Org Biomol Chem.